# N-[N-[(S)-1,3-Dicarboxypropyl]carbamoyl]-4-[^18^F]fluorobenzyl-L-cysteine

Chemical name: | N-[N-[(S)-1,3-Dicarboxypropyl]carbamoyl]-4-[^18^F]fluorobenzyl-L-cysteine
Abbreviated name: | [^18^F]DCFBC
Synonym:
Agent category: | Compound
Target: | Prostate-specific membrane antigen (PSMA), or N-acetyl α-linked acidic dipeptidase (NAALADase)
Target category: | Receptor
Method of detection: | PET
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DCFBC)]

Prostate-specific membrane antigen (PSMA) is a cell-surface glycoprotein with a molecular weight of ~100 kDa. It is a unique, type II, transmembrane-bound glycoprotein that is overexpressed on prostate tumor cells and in the neovasculature of most solid prostate tumors, but not in the vasculature of normal tissues (1, 2). It has also been detected in other tissues such as the kidney, the proximal small intestine, and the salivary glands, with minimal expression in the brain (2). PSMA was found to have N-acetyl α-linked acidic dipeptidase (NAALADase) or glutamate carboxypeptidase II (GCPII) activity (3). PSMA may play an important role in the progression of prostate cancer, glutamatergic neurotransmission, and in the absorption of folate (4). In the central nervous system, PSMA metabolizes N-acetyl-aspartyl-glutamate (NAAG), and in the proximal small intestine PSMA removes γ-linked glutamates from poly-γ-glutamate folate and folate hydrolase (2). PSMA can be used as a marker for the detection of metastatic cancers with imaging agents. Although the commercially available monoclonal antibody [^111^In]-Capromomab pendetide (^111^In-CYT-356) is in clinical use for the detection of prostate cancer, the results obtained with this antibody are not entirely reliable (5). In addition, the antibody has limited access to tumors and may produce low signal/noise ratios because the target is the intracellular domain of PSMA (6, 7). N-[N-[(S)-1,3-dicarboxypropyl]carbamoyl]-S-[^11^C]methyl-L-cysteine ([^11^C]DCMC) was evaluated for the positron emission tomography (PET) imaging of PSMA-positive tumors in an in vivo rodent model for prostate cancer (8). However, the potential widespread use of [^11^C]DCMC is limited by the short half-life of ^11^C (20 min). N-[N-[(S)-1,3-Dicarboxypropyl]carbamoyl]-4-[^18^F]fluorobenzyl-L-cysteine ([^18^F]DCFBC), an analog of DCMC, has also been studied (9).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DCFBC%20AND%20synthesis)]

(S)-2-[3-[(R)-1-Carboxy-2-mercaptoethyl]ureido]-pentanedioic acid was used as a precursor for the synthesis of [^18^F]DCFBC (9). 4-[^18^F]Fluorobenzyl bromide ([^18^F]FBB) was added to a solution of the precursor in ethanol/ammonia and heated for 10 min at 60°C. [^18^F]DCFBC was purified with high-performance liquid chromatography. However, the radiochemical purity was not reported. The time for synthesis was ~123 min from [^18^F]KF. The average non-decay-corrected yield of [^18^F]DCFBC was 16 ± 6% (n = 8) from [^18^F]FBB , with a specific radioactivity of 52 GBq/µmol (1.49 Ci/µmol) at the end of synthesis.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DCFBC%20AND%20in%20vitro)]

The binding affinity of DCFBC for PSMA was determined with the use of the NAAG peptidase assay in membranes isolated from Chinese hamster ovary cells transfected with rat GCPII (10). In this assay, 4 µM NAAG that contained trace amounts of ^3^H-NAAG was incubated with the membranes in the presence of 1–100 nM DCFBC. A 50% inhibition concentration value of 13.9 nM was determined for DCFBC (9).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DCFBC%20and%20rodentia)]

Mease et al. (9) performed biodistribution studies of [^18^F]DCFBC in nude mice bearing PSMA-positive PC-3 PIP tumor and PSMA-negative PC-3 FLU tumor xenografts. The maximum PIP tumor uptake was 8.2 ± 2.6% injected dose per gram (ID/g) at 60 min after injection, which decreased to 4.7 ± 0.9% ID/g at 120 min. The PIP/muscle ratio was 20 at 120 min. On the other hand, FLU tumors accumulated <1% ID/g at 60 and 120 min. The organ with the highest accumulation at 60 min after injection was the kidney (41.6% ID/g), followed by the urinary bladder (6.65% ID/g), liver (5.1% ID/g), blood (1.8% ID/g), and bone (1.7% ID/g). The washout from these organs was faster than the PIP tumors. The whole-body distribution of [^18^F]DCFBC was also assessed with PET imaging 20–120 min after injection. The highest radioactivity levels were visualized in the kidneys, urinary bladder, liver, and PIP tumors; FLU tumors were barely visualized. No blocking experiment was performed although the use of tumors that are PSMA positive or PSMA negative is consistent with specific binding.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DCFBC%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DCFBC%20AND%20Primates)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DCFBC%20AND%20human)]

No publication is currently available.

## NIH Support

U24 CA92871, R21 EB005324, R21 CA111982, P50 103175

## References

1 Feneley M.R., Jan H., Granowska M., Mather S.J., Ellison D., Glass J., Coptcoat M., Kirby R.S., Ogden C., Oliver R.T., Badenoch D.F., Chinegwundoh F.I., Nargund V.H., Paris A.M., Britton K.E. (2000). Imaging with prostate-specific membrane antigen (PSMA) in prostate cancer. Prostate Cancer Prostatic Dis.
2 Ghosh A., Heston W.D. (2004). Tumor target prostate specific membrane antigen (PSMA) and its regulation in prostate cancer. J Cell Biochem.
3 Luthi-Carter R., Barczak A.K., Speno H., Coyle J.T. (1998). Molecular characterization of human brain N-acetylated alpha-linked acidic dipeptidase (NAALADase). J Pharmacol Exp Ther.
4 O'Keefe, D., D. Bachich, and W.D. Heston, Prostate specific membrane antigen. Prostate cancer, biology, genetics, and the new therapeutics., ed. L. Chung, W. Issacs, and J. Simons. 2001, New Jersey: Humana Press. 307-326.
5 Ponsky L.E., Cherullo E.E., Starkey R., Nelson D., Neumann D., Zippe C.D. (2002). Evaluation of preoperative ProstaScint scans in the prediction of nodal disease. Prostate Cancer Prostatic Dis.
6 Sundaresan G., Yazaki P.J., Shively J.E., Finn R.D., Larson S.M., Raubitschek A.A., Williams L.E., Chatziioannou A.F., Gambhir S.S., Wu A.M. (2003). 124I-labeled engineered anti-CEA minibodies and diabodies allow high-contrast, antigen-specific small-animal PET imaging of xenografts in athymic mice. J Nucl Med.
7 Jain R.K. (1999). Transport of molecules, particles, and cells in solid tumors. Annu Rev Biomed Eng.
8 Foss C.A., Mease R.C., Fan H., Wang Y., Ravert H.T., Dannals R.F., Olszewski R.T., Heston W.D., Kozikowski A.P., Pomper M.G. (2005). Radiolabeled small-molecule ligands for prostate-specific membrane antigen: in vivo imaging in experimental models of prostate cancer. Clin Cancer Res.
9 Mease R.C., Dusich C.L., Foss C.A., Ravert H.T., Dannals R.F., Seidel J., Prideaux A., Fox J.J., Sgouros G., Kozikowski A.P., Pomper M.G. (2008). N-[N-[(S)-1,3-Dicarboxypropyl]carbamoyl]-4-[18F]fluorobenzyl-L-cysteine, [18F]DCFBC: a new imaging probe for prostate cancer. Clin Cancer Res.
10 Fuhrman S., Palkovits M., Cassidy M., Neale J.H. (1994). The regional distribution of N-acetylaspartylglutamate (NAAG) and peptidase activity against NAAG in the rat nervous system. J Neurochem.